# ^89^Zr-Desferrioxamine p-isothiocyanatobenzyl-anti-EGFR nanobody 7D12

Chemical name: | ^89^Zr-Desferrioxamine p-isothiocyanatobenzyl-anti-EGFR nanobody 7D12
Abbreviated name: | ^89^Zr-Df-Bz-NCS-7D12
Synonym:
Agent category: | Antibody fragment, nanobody
Target: | Epidermal growth factor receptor (EGFR, HER1)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^89^Zr
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4503491), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_001963.2) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1950) for more information about EGF.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=7D12%20nanobody)]

Epidermal growth factor (EGF) is a 53-amino acid cytokine (6.2 kDa) that is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors, including EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2; however, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 as well as HER2 are overexpressed on many solid tumor cells such as breast, non–small-cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis (7-10).

Trastuzumab, a humanized immunoglobulin G_1_ (IgG_1_) monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 (11), was labeled as ^111^In-trastuzumab (12-14). C225, an anti-EGFR (HER1), mouse-human chimeric, IgG_1_ mAb, also known as erbitux and cetuximab, was labeled as ^99m^Tc-EC-C225 (http://www.ncbi.nlm.nih.gov/books/NBK23305/) (15, 16) for imaging EGFR expression on solid tumors with the use of single-photon emission computed tomography (SPECT). However, the pharmacokinetics of the intact radiolabeled mAb, with high liver uptake and slow blood elimination, are generally not ideal for imaging (17, 18). Smaller antibody fragments, such as scFv, Fab, or F(ab')_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. Nanobodies are the smallest intact antigen-binding fragments (15 kDa) isolated from heavy-chain camelid antibodies, and they exhibit efficient and specific tumor targeting (19-21). Nanobody 7D12 was labeled with ^99m^Tc at its C-terminus hexahistidine tail as a SPECT agent for imaging EGFR expression in tumors in mice (22). For use with positron emission tomography (PET), nanobody 7D12 was conjugated with the bifunctional chelate p-isothiocyanatobenzyl-desferrioxamine (Df-Bz-NCS) and labeled with ^89^Zr (t_1/2_, 78.4 h) to form ^89^Zr-Df-Bz-NCS-7D12 for imaging HER1 expression in tumors (23).

### Related Resource Links:

- Chapters in MICAD (EGFR (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=HER1+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad), 7D12 (http://www.ncbi.nlm.nih.gov/books?term=7d12%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (EGFR (http://www.ncbi.nlm.nih.gov/gene/1956))
- Articles in Online Mendelian Inheritance in Man (OMIM) (EGFR (http://www.ncbi.nlm.nih.gov/omim/131550))
- Clinical trials (Trastuzumab (http://www.clinicaltrials.gov/ct2/results?term=Trastuzumab), cetuximab (http://www.clinicaltrials.gov/ct2/results?term=Cetuximab))
- Drug information in FDA (Trastuzumab (http://google2.fda.gov/search?q=Trastuzumab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14), cetuximab (http://google2.fda.gov/search?q=Cetuximab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=7&y=18))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=7D12%20nanobody%20and%20synthesis)]

Df-Bz-NCS-7D12 was prepared by incubation of nanobody 7D12 (125 nmol) with Df-Bz-NCS (375 nmol) in buffer (pH 9) for 30 min at 37°C (23). Df-Bz-NCS-7D12 was purified with column chromatography. There was 0.2 Df group per 7D12 molecule. For ^89^Zr-labeling, a solution of ^89^Zr (37 MBq (1 mCi)) and 7D12 (6.25–62.5 nmol) was incubated in HEPES buffer (pH 7.0) for 60 min at room temperature with labeling yields of 59%–73%. Radiochemical purity of ^89^Zr-Df-Bz-NCS-7D12 was 97%–99%. The specific activity of ^89^Zr-Df-Bz-NCS-7D12 was not reported. ^89^Zr-Df-Bz-NCS-7D12 was 97% intact after storage in buffer at 4°C and in human serum at 37°C for 24 h.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=7D12%20nanobody%20and%20in%20vitro)]

Binding experiments with 7D12 with the use of a Biacore sensor chip immobilized with extracellular domain of EGFR protein were performed (22). The K_d_ value of 7D12 was calculated to be 5.7 nM. Vosjan et al. (23) reported that the immunoreactivity of ^89^Zr-Df-Bz-NCS-7D12 was 80%–85% at 4°C using EGFR-positive human carcinoma A431 cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=7D12%20nanobody%20and%20rodentia)]

Vosjan et al. (23) performed ex vivo biodistribution studies of 0.35 MBq (0.01 mCi) ^89^Zr-Df-Bz-NCS-7D12 (3.2 nmol) in A431 tumor-bearing nude mice (n = 3/group) at 1, 2, and 3 h after injection. Accumulation into A431 tumors was 7.5 ± 1.9% injected dose/gram (ID/g) at 1 h and 7.4 ± 1.6% ID/g at 3 h. The kidney accumulation was 300% ID/g at 1 h and 300% ID/g at 3 h. The accumulation levels in other normal tissues were low (<0.5% ID/g) except for the liver, which accumulated 0.7% ID/g at 1 h. The tumor/blood ratios were 14.8, 35.2, and 42.4 at 1, 2, and 3 h after injection, respectively. No blocking studies were performed with unlabeled nanobody 7D12.

A whole-body PET static imaging study was performed in A431 tumor-bearing nude mice (n = 3) at 2–3 h after injection of 5 MBq (0.14 mCi) ^89^Zr-Df-Bz-NCS-7D12 (6.3 nmol) (23). Intense accumulation in the kidneys and urinary bladder was observed. The A431 tumors were clearly visualized. No blocking studies were performed with unlabeled nanobody 7D12.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=7D12%20nanobody%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=7D12%20nanobody%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=7D12%20nanobody%20and%20human)]

No publication is currently available.

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer: signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Schechter N.R., Yang D.J., Azhdarinia A., Kohanim S., Wendt R., Oh C.S., Hu M., Yu D.F., Bryant J., Ang K.K., Forster K.M., Kim E.E., Podoloff D.A. (2003). Assessment of epidermal growth factor receptor with 99mTc-ethylenedicysteine-C225 monoclonal antibody. Anticancer Drugs.
16 Schechter N.R., Wendt R.E., Yang D.J., Azhdarinia A., Erwin W.D., Stachowiak A.M., Broemeling L.D., Kim E.E., Cox J.D., Podoloff D.A., Ang K.K. (2004). Radiation dosimetry of 99mTc-labeled C225 in patients with squamous cell carcinoma of the head and neck. J Nucl Med.
17 Olafsen T., Wu A.M. (2010). Antibody vectors for imaging. Semin Nucl Med.
18 Wu A.M. (2009). Antibodies and antimatter: the resurgence of immuno-PET. J Nucl Med.
19 Arbabi Ghahroudi M., Desmyter A., Wyns L., Hamers R., Muyldermans S. (1997). Selection and identification of single domain antibody fragments from camel heavy-chain antibodies. FEBS Lett.
20 Desmyter A., Decanniere K., Muyldermans S., Wyns L. (2001). Antigen specificity and high affinity binding provided by one single loop of a camel single-domain antibody. J Biol Chem.
21 Muyldermans S. (2001). Single domain camel antibodies: current status. J Biotechnol.
22 Gainkam L.O., Huang L., Caveliers V., Keyaerts M., Hernot S., Vaneycken I., Vanhove C., Revets H., De Baetselier P., Lahoutte T. (2008). Comparison of the biodistribution and tumor targeting of two 99mTc-labeled anti-EGFR nanobodies in mice, using pinhole SPECT/micro-CT. J Nucl Med.
23 Vosjan M.J., Perk L.R., Roovers R.C., Visser G.W., Stigter-van Walsum M., van Bergen En Henegouwen P.M., van Dongen G.A. (2011). Facile labelling of an anti-epidermal growth factor receptor Nanobody with 68Ga via a novel bifunctional desferal chelate for immuno-PET. Eur J Nucl Med Mol Imaging.